# (S,S)-2-[α-(2-(2-[^18^F]Fluoro[^2^H_4_]ethoxy)phenoxy)benzyl]morpholine

Chemical name: | (S,S)-2-[α-(2-(2-[^18^F]Fluoro[^2^H_4_]ethoxy)phenoxy)benzyl]morpholine
Abbreviated name: | (S,S)-[^18^F]FRB-D_4_
Synonym: | (S,S)-[^18^F]Fluororeboxetine, [^18^F]FRB-D_4_
Agent Category: | Compound
Target: | Brain norepinephrine transporter (NET)
Target Category: | Transporter binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5B18F%5DFRB-D4%20OR%20%28NET%20PET%20ligand%29)]

(S,S)-2-[α-(2-(2-[^18^F]Fluoro[^2^H_4_]ethoxy)phenoxy)benzyl]morphine ((S,S)-[^18^F]FRB-D_4_) is a radioligand developed for positron emission tomography (PET) imaging of the brain adrenergic receptors (1, 2). It is a derivative of reboxetine ((RS)-2-[(RS)-2-ethoxyphenoxy)benzyl]morpholine), which is a norepinephrine (NE) transporter (NET) inhibitor, and is labeled with ^18^F, which is a positron emitter with a physical half-life (t_½_) of 109.8 min. Four hydrogens on the ethoxy side chain have been replaced with deuterium (^2^H) in an attempt to slow defluorination, which was observed in earlier studies.

Many diseases affect the sympathetic nervous system (SNS), and imaging of pathologic changes of adrenergic transmission has been an important area of PET research (3, 4). Most postganglionic sympathetic neurons in the autonomic nervous system release the neurotransmitter NE, which stimulates adrenergic receptors in various effector organs (5). There are different types and subtypes of adrenergic receptors, and they are characterized as α_1a_ to α_1c_, α_2a_ to α_2c_, and β_1_ to β_3_ (6). All NE receptors belong to the G-protein−linked receptor superfamily and mediate slow neuromodulatory postsynaptic responses. The NET is a transmembrane protein located in the adrenergic nerve terminals and is responsible for active reuptake (uptake-1) of NE released from neurons (7). NE is stored in the neuronal vesicles and is released upon stimulation. Significant expression of NET is found in major organs of the SNS, such as the heart and brain. Brain NETs are involved in various neurologic and psychiatric diseases, including depression, attention deficit hyperactivity disorder, drug addiction, and eating disorders (8). Brain NETs are also the site of action of many antidepressant drugs in the brain (9).

Molecular probes with structures closely related to NE can be used to assess the integrity of presynaptic sympathetic nerve terminals in patients with various diseases. In vivo NE synthesis is similar to dopamine synthesis, and dopamine is converted to NE by the enzyme dopamine-β-hydroxylase (6). [^123^I]-meta-Iodobenzylguanidine, [^11^C]meta-hydroxyephedrine, [^11^C]norepinephrine, and many other radioligands have been developed and used for peripheral neuronal imaging (10). However, this class of tracers is not suitable for the study of the brain NET system because they are not able to cross the normal blood-brain barrier (2). In the brain, NET levels are relatively lower compared with other receptors, such as dopamine transporters (DATs) and serotonin transporters (9). Several NET reuptake inhibitors, such as [^11^C]desipramine, have been tested, but they showed high nonspecific binding. Reboxetine is a specific NET inhibitor with a high affinity and selectivity [inhibitory concentration (IC_50_) DAT/NET = 4,000]. PET imaging has shown specific localization and favorable binding kinetics for ^11^C-labeled reboxetine derivatives [(S,S)-[^11^C]methylreboxetine ((S,S)-[^11^C]MRB)] in rats and non-human primates (11). Because of the potential advantages associated with the longer t_½_ of ^18^F, Lin et al. (1) synthesized a number of ^18^F−labeled reboxetine analogs as promising radioligands for NET imaging with PET. (S,S)-[^18^F]FRB has been shown to have high affinity and selectivity toward NET. (S,S)-[^18^F]FRB-D_4_, a tetradeuterated analog, was developed to explore the deuterium isotope effect with the intention of reducing in vivo defluorination.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28FRB%29%20AND%20synthesis)]

Lin et al. (11) described the radiosynthesis of (S,S)-[^18^F]FRB from (S,S)-N-tert-butyloxycarbonyl-2-[α-(2-hydroxyphenoxy)benzyl]morpholine (N-Boc-desethylIRB). N-Boc-desethylIRB was prepared by the N-protection of (S,S)/(R,R)-N-desethylIRB with a tert-butyloxycarbonyl (Boc) group followed by enantiomeric resolution by chiral high-performance liquid chromatobraphy (HPLC) with >99% enantiomeric purity. In the radiosynthesis, 1-bromo-2-[^18^F]fluoro[^2^H_4_]ethane ([^18^F]BFE-D_4_) was first prepared as a secondary radiolabeling synthon by the nucleophilic displacement of 2-bromoethyl triflate-D_4_ with [^18^F]F−. Briefly, 2-bromoethyl triflate-D_4_ was added to [^18^F]KF/Kryptofix 222 and vortexed for 20 s, followed by incubation at ambient temperature for 5 min. The solution was heated at 80ºC, and the volatiles were distilled into a solution of N-Boc-desethylIRB and 5 N sodium hydroxide in N,N-dimethylformamide and cooled in an acetonitrile/dry ice bath. This step produced the coupling of N-Boc-desethylIRB with [^18^F]BFE-D_4_.The mixture was then heated in an oil bath at 130ºC for 30 min. After cooling, trifluoroacetic acid was added to remove the Boc group and the mixture was heated at 75ºC for 17 min. Water was added and (S,S)-[^18^F]FRB-D_4_ was purified by high performance liquid chromatography (HPLC). After HPLC purification, (S,S)-[^18^F]FRB-D_4_ was obtained in 11−27% decay-corrected radiochemical yields from [^18^F]F−. The total synthesis time was 120 min with a radiochemical purity of >98%. The specific activity of the final product was 21−48 GBq/μmo (0.57−1.3 Ci/μmol) at the end of bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=F-%3B18%20reboxetine%20analogs)]

Lin et al. (1) determined the log P_oct_ (pH 7.4) value of FRB to be 0.91 ± 0.01 (n = 8) by traditional extraction with octanol and pH 7.4 phosphate buffer. In comparison, (S,S)-[^11^C]MRB had log P_oct_ of 1.17.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28FRB%20OR%20reboxetine%20analogs%29%20AND%20rodentia)]

Whole-body biodistribution studies of (S,S)-[^18^F]FRB-D_4_ were conducted in mice (1). At 10 min after i.v. injection of 0.185 MBq (5 μCi) (S,S)-[^18^F]FRB-D_4_, the percent injected dose per gram (%ID/g; n = 4) radioactivity levels for major organs were 15.6 ± 1.01 (liver), 10.9 ± 1.96 (intestine), 5.81 ± 0.62 (kidney), 4.71 ± 0.13 (lung), 1.58 ± 0.07 (bone), 1.08 ± 0.03 (blood), and 0.46 ± 0.01 (brain), At 2 h, these radioactivity levels changed to 5.00 ± 0.85 (liver), 32.7 ± 4.43 (intestine), 0.69 ± 0.07 (kidney), 0.38 ± 0.07 (lung), 0.25 ± 0.03 (bone), 0.22 ± 0.03 (blood), and 0.13 ± 0.01 (brain). The results showed that the radioligand was excreted through both the hepatobiliary and the renal systems. There was moderate brain radioactivity uptake and the washout was slow. In comparison, (S,S)-[^11^C]methylreboxetine had 0.53% ID brain uptake at 5 min after injection (9). (S,S)-[^18^F]FRB-D_4_ showed faster blood clearance than (S,S)-[^18^F]FRB. The bone and blood radioactivity levels of (S,S)-[^18^F]FRB-D_4_ were similar at 2 h. The radioactivity accumulation in the bone appeared to decrease continuously. In comparison, (S,S)-[^18^F]FRB showed a slight increase in bone radioactivity from 0.65 ± 0.08% ID/g at 1 h to 0.83% ID/g at 2 h. The authors suggested that this was evidence of in vivo defluorination inhibition via a deuterium isotope effect with (S,S)-[^18^F]FRB-D_4_.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5B18F%5DFRB%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28FRB%20OR%20reboxetine%20analogs%29%20AND%20%28primate%20NOT%20human%29)]

Ding et al. (12) used PET imaging to evaluate (S,S)-[^18^F]FRB-D_4_ in baboons. The radioactivity uptake of (S,S)-[^18^F]FRB-D_4_ in the baboon brain was consistent with the known NET distribution, and the uptake could be blocked by a selective NET inhibitor (1 mg/kg i.y. nisoxetine pretreatment ). The signal-to-noise ratios in the brain were similar to those of (S,S)-[^18^F]FRB. The bone radioactivity of (S,S)-[^18^F]FRB_4_ was low and did not increase with time. The blood clearance of (S,S)-[^18^F]FRB-D_4_ was faster than (S,S)-[^18^F]FRB.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5B18F%5DFRB%20AND%20human)]

No publication is currently available.

## NIH Support

NIH NIBIB EB002630, NIH NIDA DA-06278.

## References

1 Lin K.S., Ding Y.S., Kim S.W., Kil K.E. (2005). Synthesis, enantiomeric resolution, F-18 labeling and biodistribution of reboxetine analogs: promising radioligands for imaging the norepinephrine transporter with positron emission tomography. Nucl Med Biol.
2 Ding Y.S., Lin K.S., Logan J., Benveniste H., Carter P. (2005). Comparative evaluation of positron emission tomography radiotracers for imaging the norepinephrine transporter: (S,S) and (R,R) enantiomers of reboxetine analogs ([11C]methylreboxetine, 3-Cl-[11C]methylreboxetine and [18F]fluororeboxetine), (R)-[11C]nisoxetine, [11C]oxaprotiline and [11C]lortalamine. J Neurochem.
3. Konishi, J., B.A. Dwamena, M.D. Gross, B. Shapiro, T. Misaki, M. Fukunaga, J.C. Sisson, H.-Y. Oei, M. De Jong, and E. P. Krenning Endocrinology, in Molecular Nuclear Medicine, L.E. Feinendegen, W.W. Shreeve, W.C. Eckelman, Y.-W. Bahk, and H.N. Wagner Jr., Editor. 2003, Springer: New York. p. 357-409.
4. Antoni, G., T. Kihlberg, and B. Langstrom, Aspects on the synthesis of 11C-Labelled compounds, in Handbook of Radiopharmaceuticals, M.J. Welch, and C.S. Redvanly, Editor. 2003, John Wiley & Sons Ltd.: West Sussex, England. p. 141-194.
5. Sunderland, P.M., Pathophysiology. The Biologic basis for disease in adults and children, K.L. McCance, and S. E. Huether, Editor. 1994, Mosby-Year Books, Inc.: St, Louiis. p. 397-436.
6. Frey, K.A., PET study of neurochemical systems, in Positron Emission Tomography, P.E. Valk, D.L. Bailey, D.W. Townsend, and M.N. Maisey, Editors. 2002, Springer London. p. 309-327.
7 Buursma A.R., Beerens A.M., de Vries E.F., van Waarde A., Rots M.G., Hospers G.A., Vaalburg W., Haisma H.J. (2005). The Human Norepinephrine Transporter in Combination with 11C-m-Hydroxyephedrine as a Reporter Gene/Reporter Probe for PET of Gene Therapy. J Nucl Med.
8 Zahniser N.R., Doolen S. (2001). Chronic and acute regulation of Na+/Cl- -dependent neurotransmitter transporters: drugs, substrates, presynaptic receptors, and signaling systems. Pharmacol Ther.
9 Wilson A.A., Johnson D.P., Mozley D., Hussey D., Ginovart N., Nobrega J., Garcia A., Meyer J., Houle S. (2003). Synthesis and in vivo evaluation of novel radiotracers for the in vivo imaging of the norepinephrine transporter. Nucl Med Biol.
10 Langer O., Halldin C. (2002). PET and SPET tracers for mapping the cardiac nervous system. Eur J Nucl Med Mol Imaging.
11 Lin K.S., Ding Y.S. (2004). Synthesis, enantiomeric resolution, and selective C-11 methylation of a highly selective radioligand for imaging the norepinephrine transporter with positron emission tomography. Chirality.
12 Link J.M., Synovec R.E. (1999). Whole-column radioactivity detection: simultaneous separation and enhanced detectability. Anal Chem.